# Indocyanine green derivative 02-2-deoxy-D-glucose

Chemical name: | Indocyanine green derivative 02-2-deoxy-D-glucose
Abbreviated name: | ICG-Der-02-2DG
Synonym:
Agent category: | Compound
Target: | Glucose transporters, hexokinases
Target category: | Transporter, enzyme
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | ICG-Der-02
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive complement to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (5-8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (9). There are four HKs in mammalian tissues (HKI–HKIV). HKI, HKII, and HKIII have molecular weights of ~100,000 each; HKI is found mainly in the brain, and HKII is insulin-sensitive and is found in adipose and muscle cells. HKIII is found mainly in the liver and lung. HKIV, also known as glucokinase, has a molecular weight of ~50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (10), which was detected in tumors from patients with lung, gastrointestinal, and breast cancers. The HKs, by converting glucose to glucose-6-phosphate, help maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1–GLUT13) (11). GLUT1 is considered to be the main transporter of glucose uptake. GLUT4 and HKII are the major transporter and HK isoform in skeletal muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2DG) was first developed to inhibit glucose utilization by cancer cells (12). HKs phosphorylate 2DG to 2DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/books/NBK23335/)) was later developed for use in molecular imaging studies (13). FDG is moved into cells by glucose transporters and is then phosphorylated by HK to FDG-6-phosphate. FDG-6-phosphate cannot be metabolized further in the glycolytic pathway and remains in the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells and activated cells enhance the uptake of FDG in these cells relative to normal cells. Positron emission tomography (PET) with [^18^F]FDG has been used to assess alterations in glucose metabolism in brain, cancers, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, and infectious, autoimmune, and inflammatory diseases (14-19). Various NIR dyes (such as Cypate, Cy5.5, and IRDye800CW) were conjugated to 2DG (20-22) as optical imaging agents for in vivo imaging of glucose utilization in tumors in mice. ICG derivative 02 (ICG-Der-02) contains one carboxyl functional group for covalent conjugation to the amino group of biomolecules. ICG-Der-02 is a hydrophilic dye. Guo et al. (23) evaluated ICG-Der-02-2DG for in vivo NIR optical imaging in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (hexokinase (http://www.ncbi.nlm.nih.gov/books?term=(hexokinase%20OR%20hexokinases)%20AND%20micad%5Bbook%5D), glucose transporter (http://www.ncbi.nlm.nih.gov/books?term=glucose%20transporters%20%20AND%20micad%5Bbook%5D), ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (hexokinase (http://www.ncbi.nlm.nih.gov/gene?term=hexokinase%20human), GLUT1 (http://www.ncbi.nlm.nih.gov/gene/6513))
- Articles in Online Mendelian Inheritance in Man (OMIM) (hexokinase (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hexokinase%5BAll+Fields%5D), GLUT1 (http://www.ncbi.nlm.nih.gov/omim/138140))
- Clinical trials (ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG), [^18^F]FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA (ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8), [^18^F]FDG (http://google2.fda.gov/search?q=%5B18F%5DFDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+synthesis)]

ICG-Der-02-N-hydroxysuccinimide ester (0.0128 mmol) was reacted with 2-amino-2-DG (0.064 mmol) for 18 h at room temperature in sodium phosphate buffer (pH 9) (23). ICG-Der-02-2DG was purified with high-performance liquid chromatography and verified with mass spectroscopy. There is one dye molecule per ICG-Der-02-2DG molecule. The yield of ICG-Der-02-2DG was ~32%, with 92% purity. ICG-Der-02-2DG displayed spectral properties similar to those of ICG-Der-02, with maximum absorption at 783 nm and maximum emission at 811 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+in+vitro)]

In vitro uptake studies of rhodamine-2DG (RhB-2DG) were performed with MCF-7/estradiol, U87MG, and MCF-7 tumor cells in culture, showing that high, medium, and low fluorescence intensity correlated respectively with the GLUT1 expression levels (23). Fluorescence confocal microscopy showed that RhB-2DG accumulated in the cytoplasm of the tumor cells. Excess 2DG was able to block the fluorescence signal in the cytoplasm. Rhodamine was used because the investigators do not have confocal fluorescence microcopy with NIR capability.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+rodentia)]

Guo et al. (23) performed in vivo NIR fluorescence imaging studies in nude mice (n = 5) bearing GLUT1-expressing MCF-7/estradiol xenografts at 0.5–48 h after intravenous injection of ICG-Der-02-2DG (10 nmol per mouse). ICG-Der-02-2DG accumulated mainly in the tumors, with a peak tumor/muscle ratio of 8.87 ± 0.31 at 4 h. The tumor/muscle ratio gradually decreased to ~7 at 48 h. Among the normal tissues, only kidneys exhibited strong fluorescence signal, indicative of renal excretion of ICG-Der-02-2DG. Ex vivo NIR fluorescence imaging showed that the tumors exhibited the highest fluorescence intensity (tissue/background ratio, ~17), followed by the kidney (~12), liver (~5), lung (~4), spleen (~3), intestine (~2), and heart (~2). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ICG-Der-02-2DG+human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
6 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
7 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
8 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
9 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
10 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
11 Wood I.S., Trayhurn P. (2003). Glucose transporters (GLUT and SGLT): expanded families of sugar transport proteins. Br J Nutr.
12 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
13 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
14 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
15 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
16 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
17 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
18 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
19 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
20 Kovar J.L., Volcheck W., Sevick-Muraca E., Simpson M.A., Olive D.M. (2009). Characterization and performance of a near-infrared 2-deoxyglucose optical imaging agent for mouse cancer models. Anal Biochem.
21 Cheng Z., Levi J., Xiong Z., Gheysens O., Keren S., Chen X., Gambhir S.S. (2006). Near-infrared fluorescent deoxyglucose analogue for tumor optical imaging in cell culture and living mice. Bioconjug Chem.
22 Chen Y., Zheng G., Zhang Z.H., Blessington D., Zhang M., Li H., Liu Q., Zhou L., Intes X., Achilefu S., Chance B. (2003). Metabolism-enhanced tumor localization by fluorescence imaging: in vivo animal studies. Opt Lett.
23 Guo J., Du C., Shan L., Zhu H., Xue B., Qian Z., Achilefu S., Gu Y. (2012). Comparison of near-infrared fluorescent deoxyglucose probes with different dyes for tumor diagnosis in vivo. Contrast Media Mol Imaging.